# ^99m^Tc-Labeled acetylated, 2,3,5-triiodobenzoic acid- and diethylenetriamine pentaacetic acid-conjugated, and PEGylated ethylenediamine-core generation 4 polyamidoamine dendrimers

Chemical name: | ^99m^Tc-Labeled acetylated, 2,3,5-triiodobenzoic acid- and diethylenetriamine pentaacetic acid-conjugated, and PEGylated ethylenediamine-core generation 4 polyamidoamine dendrimers | [image]
Abbreviated name: | ^99m^Tc-G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Non-targeted | [image]
Target Category: | Non-targeted | [image]
Method of detection: | Multimodality imaging (SPECT and CT) | [image]
Source of signal / contrast: | ^99m^Tc and iodine (2,3,5-triiodobenzoic acid (TIBA)) | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Schematic structure of ^99m^Tc-G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] by Criscione et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=multimodal%20imaging%20and%20dendrimers)]

^99m^Tc-Labeled acetylated, 2,3,5-triiodobenzoic acid (TIBA)- and diethylenetriamine pentaacetic acid (DTPA)-conjugated, and PEGylated ethylenediamine-core generation 4 polyamidoamine dendrimers (G4 PAMAM), abbreviated as ^99m^Tc-G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_], is a blood pool multimodal agent synthesized by Criscione et al. for single-photon emission computed tomography (SPECT)/computed tomography (2) (1).

In the recent years, the fact that imaging modalities with high sensitivity have relatively poor resolution, while those with high resolution have relatively poor sensitivity, has triggered the integration of multiple modalities and the use of hybrid instrument technology in imaging (3, 4). This has also boosted the development of multimodal imaging agents, which further enhances the benefits of hybrid technology, allowing better characterization of diseases and disease processes (5-7). However, it is still challenging to incorporate enough labels for detection by the relatively low-sensitive modalities and to select an appropriate radionuclide in a radiotracer-based imaging approach in the development of multimodal agents (1).

Criscione et al. synthesized a radiolabeled, multimodal contrast agent, ^99m^Tc-G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_], for preclinical microSPECT/CT imaging (1). The design of this agent is based on the G4 PAMAM dendrimers, which were used as the core structure of the multimodal agent. Dendrimers have been selected for two main reasons. First, their well-defined, multifunctional surface (64 primary amines) offers the ability to conjugate several different moieties with negligible steric hindrance. Second, dendrimer-based contrast agents have already been successfully designed and examined with different imaging modalities (1, 8, 9). However, PAMAM dendrimers have a highly cationic surface, which limits their water solubility and can cause hemolysis in humans (1). Dendrimers also have a relatively short circulation time when they are used for developing blood pool imaging agents. To overcome these problems, Criscione et al. partially acetylated the dendrimer surface to reduce the positive surface charge and PEGylated the remaining surface amines to enhance the circulation time and limit the clearance by the reticuloendothelial system (1). These modifications provided dendrimers the desired water solubility, long intravascular residence time, and predominant renal clearance (1). To induce the dendrimer construct's multimodal capability, Criscione et al. selected TIBA and ^99m^Tc-DTPA for X-ray attenuation and radioactive signal, respectively (1). TIBA possesses X-ray attenuation properties similar to those of the clinically used, small-molecule triiodobenzoic acid derivative Omnipaque 350. The studies by Criscione et al. have also shown that sufficient iodine weight percent for effective X-ray attenuation without sacrificing aqueous solubility can be achieved by conjugating TIBA to dendrimers (1). The acyclic chelator DTPA was used to chelate tin(II)-reduced ^99m^Tc because of its established chemistry and stability. In vitro and animal studies have confirmed the potential usefulness of this multimodal agent in the quantification of intramyocardial blood volume and blood flow (1).

### Related Resource Links:

Multimodal imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=multimodal+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Drug information for Omnipaque 350 at Drugs@FDA (http://www.accessdata.fda.gov/scripts/cder/drugsatfda/index.cfm?fuseaction=Search.Overview&DrugName=OMNIPAQUE%20350&CFID=402127&CFTOKEN=a62439b4b7b1a6cc-F3288437-5056-9B01-A38FCCC660804165)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21851119)]

Criscione et al. described the synthesis of ^99m^Tc-G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] in detail (1). The synthesis could be roughly divided into five steps. The G4 dendrimers were partially acetylated with sulfosuccinimidyl acetate to generate acetylated dendrimers (G4-[Ac]). Then TIBA was covalently conjugated to G4-[Ac] through the surface amines to generate G4-[[Ac]-TIBA]. To chelate the nuclear probe ^99m^Tc, 1-(4-isothiocyanatobenzyl)diethylenetriamine pentaacetic acid (p-SCN-Bn-DTPA) was coupled to the primary surface amines of the dendrimer via isothiocyanate linkage. This step resulted in the product G4-[[[Ac]-TIBA]-DTPA]. G4-[[[Ac]-TIBA]-DTPA] was subsequently PEGylated with succinimidyl-(N-methyl-dodecaethylene glycol)ester (mPEG_12_) to generate the G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_]. The chemical yields of the intermediate products were 97% for G4-[Ac], 82% for G4-[[Ac]-TIBA], 89% for G4-[[[Ac]-TIBA]-DTPA], and 83% for G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_]. Finally, ^99m^Tc-labeling was completed with the reaction of G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] (50 mg for imaging purposes and 20 mg for biodistribution studies) and ^99m^TcO_4_^–^ (18.5 MBq (500 μCi)) for 2 min (for imaging purposes) or for 10 min (for biodistribution studies) at 25ºC. The reaction mixture was directly used for studies without further purification. The radiochemical purity was >80%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21851119)]

Criscione et al. characterized the intermediate products with ^1^H nuclear magnetic resonance (NMR) spectroscopy and dynamic light scattering (1). The results showed that G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] had 3 remaining primary amines, 35 coupled acetyl groups, ~15 TIBA moieties, 4 DTPA, and 7 mPEG_12_. The hydrodynamic diameter and molecular weight of G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] were 12.37 ± 6.09 nm and 19,762, respectively.

The X-ray attenuation property of G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] was analyzed with serially diluted G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] in deionized water using microCT imaging (1). A linear attenuation versus the iodine concentration curve, an essential criterion for X-ray contrast agents, was obtained for G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_]. The extrapolated iodine concentrations in G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] were consistent with the estimated iodine weight percent (~19% wt) determined with ^1^H NMR.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21851119)]

The biodistribution and pharmacokinetics of ^99m^Tc-G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] were evaluated in C57BL/6 mice after injection of 4.255 MBq (115 μCi) of the agent. Mice were euthanized at 0.5, 1, 2, 4, and 6 h after injection (n = 4 mice/time point) (1). Blood samples and organs were harvested, and radioactivity was counted. The analysis showed that the agent’s half-life was 0.72 h (43 min), and the agent was cleared from the blood pool predominantly by the kidneys.

The efficacy of G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] as a blood pool CT contrast agent was assessed in C57BL/6 mice with serial cardiac microCT after intravenous injection of either 1.27 µmol (n = 2 mice) or 2.53 µmol (n = 2 mice) of the agent (1). Intravascular and intraventricular enhancement with an excellent contrast/noise ratio in the right and left ventricles of the heart was observed with both doses. The enhancement persisted for >90 min after injection.

The multimodal capability of G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] was assessed in mice euthanized 5 min after injection of 16.28 ± 0.96 MBq (440 ± 26 μCi) ^99m^Tc-G4-[[[[Ac]-TIBA]-DTPA]-mPEG_12_] (n = 5 mice) (1). Post-mortem microSPECT/CT imaging revealed intravascular retention, minimal liver accumulation, and substantial colocalization of the radioactivity and the dendritic iodinated contrast within the intravascular and intraventricular cavities in the absence of motion artifacts. These results demonstrate the potential usefulness of the agent as a blood pool multimodal agent and also provide evidence for the formation of a sufficiently pure and stable chelate, as either colloidal or free hydrolyzed/reduced ^99m^Tc would be cleared predominantly by the liver.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed]

No references are currently available.

## References

1 Criscione J.M., et al. (2011). Development and application of a multimodal contrast agent for SPECT/CT hybrid imaging. Bioconjug Chem.
2 Hoekzema E., et al. (2011). [(11)C]-DASB microPET imaging in the aged rat: frontal and meso-thalamic increases in serotonin transporter binding. Exp Gerontol.
3 Cherry S.R. (2006). Multimodality in vivo imaging systems: twice the power or double the trouble?. Annu Rev Biomed Eng.
4 Cherry S.R. (2009). Multimodality imaging: beyond PET/CT and SPECT/CT. Semin Nucl Med.
5 Lee S., Chen X. (2009). Dual-modality probes for in vivo molecular imaging. Mol Imaging.
6 Louie A. (2010). Multimodality imaging probes: design and challenges. Chem Rev.
7 Jennings L.E., Long N.J. (2009). 'Two is better than one'--probes for dual-modality molecular imaging. Chem Commun (Camb).
8 Mintzer M.A., Grinstaff M.W. (2011). Biomedical applications of dendrimers: a tutorial. Chem Soc Rev.
9 Cheng Y., et al. (2011). Design of biocompatible dendrimers for cancer diagnosis and therapy: current status and future perspectives. Chem Soc Rev.